# ^99m^Tc-2-Methoxyisobutylisonitrile

Chemical name: | ^99m^Tc-2-Methoxyisobutylisonitrile
Abbreviated name: | ^99m^Tc-MIBI
Synonym: | ^99m^Tc-hexakismethoxyisobutylisonitrile, ^99m^Tc-Sestamibi
Agent category: | Compound
Target: | P-glycoprotein, MDR-1, mitochondria
Target category: | Transporter
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22Technetium%20Tc%2099m%20Sestamibi%22%5BMeSH%5D)]

Lipophilic cations are capable of passive diffusion into the cytoplasm and mitochondria of cells in response to a large negative plasma- and mitochondrial- membrane potentials. ^99m^Tc-2-methoxyisobutylisonitrile (MIBI) was taken up into both normal and malignant cells being driven by metabolic demand and membrane potential (1) (2) ^99m^Tc-MIBI was originally developed as a myocardial perfusion imaging agent and subsequently as tumor imaging agent. The uptake of ^99m^Tc-MIBI is also used as a biomarker for cellular metabolism in malignant tumors.

One of the mechanisms of cells to escape the cytotoxic effects of chemotherapeutic agents, such as Adriamycin, Vinca alkaloids, epipodophyllotoxins, actinomycin D, and taxol, is to limit their presence inside the cells by a multidrug resistance (MDR-1) gene protein. The MDR-1 gene encodes a transmembrane P-glycoprotein (Pgp) as a multidrug transporter that is capable of actively pumping a variety of agents out of the cells (3). Overexpression of Pgp in tumor cells leads to resistance to anticancer drugs (4). MIBI is a transport substrate of Pgp in a variety of tumor cells (5). Another mechanism of tumor cells to escape anticancer treatments is to acquire a defective apoptotic program. Apoptosis is a highly regulated, multistep process involving the mitochondria. Bcl-2 is an integral protein on the outer mitochondrial membrane, nuclear membrane, and endoplasmic reticulum. Cancer cells have been found to have a high level of Bcl-2, which is anti-apoptotic. Overproduction of the Bcl-2 protein also prevents cell death induced by nearly all cytotoxic anticancer drugs and radiation (6, 7). MIBI is being used as a myocardial perfusion imaging agent in clinical use to assess the risk of future cardiac events. It is also used as a tumor-imaging agent in breast, lung, thyroid, and brain cancers.

### Related Resource Links:

- Chapters in MICAD (P-glycoprotein (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=P-glycoprotein%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (P-glycoprotein (http://www.ncbi.nlm.nih.gov/gene/5243))
- Articles in OMIM (P-glycoprotein (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=P-glycoprotein%5BAll+Fields%5D))
- Clinical trials (P-glycoprotein (http://www.clinicaltrials.gov/ct2/results?term=P-glycoprotein), ^99m^Tc-MIBI (http://www.clinicaltrials.gov/ct2/results?term=Sestamibi))
- Drug information in FDA (^99m^Tc-MIBI (http://google2.fda.gov/search?q=99mTc-sestamibi+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=16))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22Technetium%20Tc%2099m%20Sestamibi%22%5BMeSH%5D%20AND%20synthesis)]

^99m^Tc-MIBI was prepared by reacting 2-methoxyisobutylisonitrile with ^99m^Tc-O_4_ˉ in the presence of sodium dithionite. Radiochemical purity was greater than 98% after Sep-Pak purification (8). A commercial lyophilized kit is available (9).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22Technetium%20Tc%2099m%20Sestamibi%22%5BMeSH%5D%20AND%20in%20vitro)]

Cultured chick embryo heart cells, myocytes, accumulated [^99m^Tc]MIBI with a half-time of 9.3 min reaching a plateau at 40 min. An apparent K_d_ of 7 x 10^-5^M was assessed. The uptake could be inhibited by a metabolic inhibitor, iodoacetate, with an IC_50_ of 5 x 10^-6^M (10). Subcellular analysis of ^99m^Tc-MIBI in isolated rat hearts showed that about 90% of MIBI activity was associated with the mitochondria (11). A panel of eight human carcinoma cell lines and one leukemia cell line was incubated with ^99m^Tc-MIBI for one hour. The uptakes were varied from 5-28% of the activity in the external media. In contrast, normal Chinese hamster lung fibroblasts and human peripheral blood mononuclear leukocytes did not exhibit a uptake of more than 2% (12). The uptake was dependent on energy, plasma membrane potential and mitochondria membrane potential.

## Animal studies

### Rodent Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22Technetium%20Tc%2099m%20Sestamibi%22%5BMeSH%5D%20AND%20rodentia%20Not%20in%20vitro)]

Rats showed a good uptake in the heart, liver, kidneys, and intestine with low uptake in the lungs after 30-60 min of injection of [^99m^Tc]MIBI (9, 13). Various tumor models in rodents were evaluated to determine the role of MDR and Bcl-2 in the uptake of [^99m^Tc]MIBI by cancer cells [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22Technetium%20Tc%2099m%20Sestamibi%22%5BMeSH%5D%20AND%20%28%22rodentia%22%5BMeSH%20Terms%5D%20OR%20rodentia%5BText%20Word%5D%29%20AND%20tumor%5BText%20Word%5D)]. Myocardial perfusion studies were performed in mice and rats with [^99m^Tc]MIBI to determine the actual infarct size [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22Technetium%20Tc%2099m%20Sestamibi%22%5BMeSH%5D%20AND%20%22rodentia%22%5BMeSH%20Terms%5D%20AND%20%22myocardium%22%5BMeSH%20Terms%5D)].

### Other Non-Primate Mammal Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22Technetium%20Tc%2099m%20Sestamibi%22%5BMeSH%5D%20AND%20%22animals%22%5BMeSH%5D%20NOT%20%22rodentia%22%5BMeSH%5D%20NOT%20%22primates%22%5BMeSH%5D)]

Myocardial blood flow was found to be linearly related to ^99m^Tc-MIBI uptake in dogs with minimal washout and redistribution (14). Excellent static myocardial images were obtained for several hours. Many myocardial perfusion and infraction experiments were performed in rabbits [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22Technetium%20Tc%2099m%20Sestamibi%22%5BMeSH%5D%20AND%20%28%22rabbits%22%5BMeSH%20Terms%5D%20OR%20rabbits%5BText%20Word%5D%29)], pigs [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22Technetium%20Tc%2099m%20Sestamibi%22%5BMeSH%5D%20AND%20%28%22swine%22%5BMeSH%20Terms%5D%20OR%20pigs%5BText%20Word%5D%29)] and dogs [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22Technetium%20Tc%2099m%20Sestamibi%22%5BMeSH%5D%20AND%20%22dogs%22%5BMeSH%20Terms%5D%20AND%20%22myocardium%22%5BMeSH%5D)] using ^99m^Tc-MIBI.

### Non-Human Primate Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22Technetium%20Tc%2099m%20Sestamibi%22%5BMeSH%5D%20AND%20primates%20not%20humans)]

Myocardial images with ^99m^Tc-MIBI of the monkey showed good contrast and low wash-out (9). There was a rapid blood clearance and hepatic excretion.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22Technetium%20Tc%2099m%20Sestamibi%22%5BMeSH%5D%20AND%20human)]

[^99m^Tc]MIBI is used as an important myocardial perfusion imaging agent to evaluate coronary artery disease and myocardial infraction [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22Technetium%20Tc%2099m%20Sestamibi%22%5BMeSH%5D%20AND%20%22humans%22%5BMeSH%5D%20AND%20%22myocardium%22%5BMeSH%5D)]. [^99m^Tc]MIBI is readily accumulated in the heart. Human dosimetry was estimated from 17 normal volunteers (15). The large and small intestines received the highest dose of radioactivity, followed by the gallbladder, urinary bladder, and kidneys. The total body absorbed dose was 4.4 mGy/GBq (16 mrad/mCi). Many clinical studies have been performed to correlate [^99m^Tc]MIBI uptake or clearance with histological, molecular, and biochemical markers of various cellular processes, including apoptosis, proliferation, Pgp expression, and angiogenesis. The early tracer uptake reflects the mitochondrial status, which is affected by both apoptosis and proliferation. On the other hand, the tracer clearance reflects the activity of drug transporters such as Pgp. The uptake and clearance of [^99m^Tc]MIBI by cancer cells may determine tumor response to anticancer treatment as shown in breast cancer patients (16). In addition to tumor localization, [^99m^Tc]MIBI has been used to predict and monitor sensitivity to anticancer treatments in breast cancer [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22Technetium%20Tc%2099m%20Sestamibi%22%5BMeSH%5D%20AND%20%22humans%22%5BMeSH%5D%20AND%20%22breast%20neoplasms%22%5BMeSH%5D)], lung cancer [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22Technetium%20Tc%2099m%20Sestamibi%22%5BMeSH%5D%20AND%20%22humans%22%5BMeSH%5D%20AND%20%22lung%20neoplasms%22%5BMeSH%5D)], thyroid cancer [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22Technetium%20Tc%2099m%20Sestamibi%22%5BMeSH%5D%20AND%20%22hominidae%22%5BMeSH%5D%20AND%20%22thyroid%20neoplasms%22%5BMeSH%5D)], hepatocellular carcinoma [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22Technetium%20Tc%2099m%20Sestamibi%22%5BMeSH%5D%20AND%20%22humans%22%5BMeSH%5D%20AND%20%22liver%20neoplasms%22%5BMeSH%5D)], lymphoma [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22Technetium%20Tc%2099m%20Sestamibi%22%5BMeSH%5D%20AND%20%22humans%22%5BMeSH%5D%20AND%20%22lymphoma%22%5BMeSH%5D)], and gastric cancer (17).

## References

1 Chernoff D.M., Strichartz G.R., Piwnica-Worms D. (1993). Membrane potential determination in large unilamellar vesicles with hexakis(2-methoxyisobutylisonitrile)technetium(I). Biochim Biophys Acta.
2 Chiu M.L., Kronauge J.F., Piwnica-Worms D. (1990). Effect of mitochondrial and plasma membrane potentials on accumulation of hexakis (2-methoxyisobutylisonitrile) technetium(I) in cultured mouse fibroblasts. J Nucl Med.
3 Gottesman M.M., Pastan I. (1993). Biochemistry of multidrug resistance mediated by the multidrug transporter. Annu Rev Biochem.
4 Gottesman M.M., Hrycyna C.A., Schoenlein P.V., Germann U.A., Pastan I. (1995). Genetic analysis of the multidrug transporter. Annu Rev Genet.
5 Piwnica-Worms D., Rao V.V., Kronauge J.F., Croop J.M. (1995). Characterization of multidrug resistance P-glycoprotein transport function with an organotechnetium cation. Biochemistry.
6 Aloj L., Zannetti A., Caraco C., Del Vecchio S., Salvatore M. (2004). Bcl-2 overexpression prevents 99mTc-MIBI uptake in breast cancer cell lines. Eur J Nucl Med Mol Imaging.
7 Reed J.C., Miyashita T., Takayama S., Wang H.G., Sato T., Krajewski S., Aime-Sempe C., Bodrug S., Kitada S., Hanada M. (1996). BCL-2 family proteins: regulators of cell death involved in the pathogenesis of cancer and resistance to therapy. J Cell Biochem.
8 Piwnica-Worms D., Kronauge J.F., Holman B.L., Davison A., Jones A.G. (1989). Comparative myocardial uptake characteristics of hexakis (alkylisonitrile) technetium(I) complexes. Effect of lipophilicity. Invest Radiol.
9 Pandey P.M., Sachdev S.S., Ramamoorthy N., Lal R., Ranganatha D.K., Narasimhan S., Oommen R., Gunasekaran S., Nair N.A. (1997). Formulation and evaluation of a two-components lyophilized kit for Tc-sestamibi: transchelation preparation of Tc-99m-sestamibi. Nucl Med Biol.
10 Piwnica-Worms D., Kronauge J.F., Delmon L., Holman B.L., Marsh J.D., Jones A.G. (1990). Effect of metabolic inhibition on technetium-99m-MIBI kinetics in cultured chick myocardial cells. J Nucl Med.
11 Carvalho P.A., Chiu M.L., Kronauge J.F., Kawamura M., Jones A.G., Holman B.L., Piwnica-Worms D. (1992). Subcellular distribution and analysis of technetium-99m-MIBI in isolated perfused rat hearts. J Nucl Med.
12 Delmon-Moingeon L.I., Piwnica-Worms D., Van den Abbeele A.D., Holman B.L., Davison A., Jones A.G. (1990). Uptake of the cation hexakis(2-methoxyisobutylisonitrile)-technetium-99m by human carcinoma cell lines in vitro. Cancer Res.
13 Bouquillon S., Coulais Y., Dartiguenave M., Tafani J.A., Guiraud R. (1995). Synthesis, characterization and biodistribution of a new technetium-99m complex with trimethylsilylmethylisonitrile. Comparison with 99mTc-TBI and 99mTc-MIBI. Nucl Med Biol.
14 Okada R.D., Glover D., Gaffney T., Williams S. (1988). Myocardial kinetics of technetium-99m-hexakis-2-methoxy-2-methylpropyl-isonitrile. Circulation.
15 Wackers F.J., Berman D.S., Maddahi J., Watson D.D., Beller G.A., Strauss H.W., Boucher C.A., Picard M., Holman B.L., Fridrich R. (1989). Technetium-99m hexakis 2-methoxyisobutyl isonitrile: human biodistribution, dosimetry, safety, and preliminary comparison to thallium-201 for myocardial perfusion imaging. J Nucl Med.
16 Del Vecchio S., Salvatore M. (2004). 99mTc-MIBI in the evaluation of breast cancer biology. Eur J Nucl Med Mol Imaging.
17 Kawata K., Kanai M., Sasada T., Iwata S., Yamamoto N., Takabayashi A. (2004). Usefulness of 99mTc-sestamibi scintigraphy in suggesting the therapeutic effect of chemotherapy against gastric cancer. Clin Cancer Res.